# PEGylated 4-[^18^F]fluorobenzoyl-NAVPNLRGDLQVLAQKVART

Chemical name: | PEGylated 4-[^18^F]fluorobenzoyl- NAVPNLRGDLQVLAQKVART
Abbreviated name: | PEGylated [^18^F]FBA-A20FMDV2
Synonym: | [^18^F]FBA-PEG_28_-A20FMDV2; [^18^F]FBA-(PEG_28_)_2_-A20FMDV2
Agent Category: | Peptide ligand
Target: | Integrin α_v_β_6_
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=integrins+and+cancer)]

Integrins belong to the seven transmembrane protein receptor families, and the receptor is composed of an α (24 forms) and a β (8 forms) subunit that can associate in different combinations to produce at least 24 types of heterodimeric molecules as described by Bandyopadhyay and Raghvan (1). The integrin receptor activity is influenced by the type of constitutive α and β subunit combination, and, depending on the combination, the receptor can promote cell adhesion to fibronectin, laminins, or collagens (2). Among the various types of integrin receptors, the α_v_β_6_ combination is of particular interest to investigators because it is not expressed in normal tissue and is upregulated during wound healing and inflammation (3), as well as in certain cancers (4-6). Because of its overexpression in certain cancers (1), this integrin receptor has been targeted for the diagnosis (4, 7) and treatment of various neoplasias (1, 8). Also, overexpression of the α_v_β_6_ integrin has been suggested to indicate a poor prognosis for patients suffering from different cancers (4, 7, 9). In order to develop methods for the early detection of cancers that express the α_v_β_6_ integrin receptors, investigators have attempted the use of non-invasive molecular imaging techniques (using different modalities such as magnetic resonance imaging, optical and ultrasound imaging, etc.) to detect and determine the expression of this receptor in different cancers so as to develop a suitable treatment regimen that could improve the prognosis for patients (10).

Recently, an ^18^F-labeled peptide derived from the foot and mouth disease virus, [^18^F]fluorobenzoyl-A20FMDV2 ([^18^F]FBA-A20FMDV2; for more information regarding this peptide, see Hausner and DiCara et al. (11)), was used for the selective imaging of tumors that overexpress the α_v_β_6_ integrin with positron emission tomography (PET) (11). Although the labeled peptide could be used for imaging, this radiotracer was considered unsuitable for general use by the investigators due to poor uptake and label retention by the tumors (12). In an effort to improve the pharmacokinetics of A20FMDV2, the peptide was conjugated with monodispersed polyethylene glycol (PEG) polymers to generate mono- and diPEGylated versions, PEG_28_-A20FMDV2 and (PEG_28_)_2_-A20FMDV2, of the peptide (12). The PEGylated peptides were then labeled with ^18^F as before to obtain two radiotracers: [^18^F]FBA-PEG_28_-A20FMDV2 and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2. The biodistribution and imaging characteristics of the mono- and diPEGylated radiopeptides were investigated in mice bearing the α_v_β_6_ integrin–expressing human xenograft tumors and compared with the parent ^18^F-labeled peptide (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFAB-PEG28-A20FMDV2+synthesis)]

The synthesis of mono- and diPEGylated FBA-A20FMDV2 was described by Hausner and Abbey et al. (12). The compounds were characterized with the use of matrix-assisted laser desorption/ionization mass spectrometry. The labeling of FBA-PEG_28_-A20FMDV2 with ^18^F, to obtain [^18^F]FBA-PEG_28_-A20FMDV2, was done as detailed elsewhere (12, 13). The decay-corrected radiochemical yield and purity of the labeled compound were reported to be 6.4 ± 2.0% and 97%, respectively. The specific activity of [^18^F]FBA-PEG_28_-A20FMDV2 was >37 GBq/μmol (>1 Ci/μmol). The stability of neither the non-radioactive nor the labeled compound under in vitro or in vivo conditions was reported.

The synthesis of [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 was also done as detailed by Hausner and Abbey et al. (12). The decay-corrected radiochemical yield of [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 was 5.4 ± 2.5% with a purity of >97%. The specific activity of [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 was >37 GBq/μmol (>1 Ci/μmol), and the stability of neither the non-radioactive nor the labeled compound was reported.

The parent ^18^F-labeled compound was synthesized as described earlier (11).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFAB-PEG28-A20FMDV2+in+vitro)]

The binding and internalization of [^18^F]FBA-(PEG_28_)_n_-A20FMDV2 was studied using cultured DX3puroβ6 cells (stably transduced with, and expressing high levels of, α_v_β_6_ integrin DNA), DX3puro cells (negative controls; do not express any α_v_β_6_ integrin), and BxPC-3 cells (positive controls; a human pancreatic cancer cell line that constitutively expresses the α_v_β_6_ integrin receptor) (12). Binding of the respective labeled peptide ligands to the different cell lines was reported to depend on the level of α_v_β_6_ integrin expression by each cell type. The binding of [^18^F]FBA-A20FMDV2, [^18^F]FBA-PEG_28_-A20FMDV2, and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 to the DX3puroβ6 and BxPC-3 cells was 5.3 ± 0.8 and 9.7 ± 1.2%, 73.5 ± 1.3 and 68.9 ± 0.2%, and 38.5 ± 1.7 and 25.8 ± 0.6%, respectively. Almost 66% of the bound radioactive PEGylated compounds were internalized by the cells; however, <50% of the bound [^18^F]FBA-A20FMDV2 was internalized by the cells. Incubation of DX3puroβ6 cells with [^18^F]FBA-PEG_28_-A20FMDV2 in presence of the unlabeled compound (≥1 μmol/L) was shown to completely block binding of the radiotracer to the cells.

The binding of [^18^F]FBA-PEG_28_-A20FMDV2 in the presence of transforming growth factor β1 human latency-associated peptide (LAP), another high affinity ligand for the α_v_β_6_ integrin receptor, to the DX3puroβ6 and BxPC-3 cells was also studied (12). With both cell lines, >75% of the radiotracer remained bound in the presence of LAP versus 100% in the absence of LAP.

As determined with ELISA assays, the 50% inhibitory concentrations (IC_50_) of [^18^F]FBA-A20FMDV2, [^18^F]FBA-PEG_28_-A20FMDV2, and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 for the α_v_β_6_ integrin were reported to be 3 ± 1, 6 ± 4, and 5 ± 2 nmol/L, respectively (12). This suggested that the parent and the PEGylated compounds had a similar affinity for the integrin receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFAB-PEG28-A20FMDV2+rodentia)]

Two different animal models were used to investigate the biodistribution of the ^18^F-labeled non-, mono-, and diPEGylated versions of FBA-A20FMDV2 (12). For these studies, three mice were used per time point per labeled compound per model. For the first animal model, mice bearing paired xenograft tumors derived from the DX3puroβ6 and DX3puro cells were used as described (11). PEGylation of FBA-A20FMDV2 resulted in an improved retention of radioactivity by the DX3puroβ6 tumors. Compared with [^18^F]FBA-A20FMDV2, which had a retention of 0.66 ± 0.09 and 0.06 ± 0.00% injected dose/gram tissue (% ID/g) at 1 and 4 h, respectively, the retention of [^18^F]FBA-PEG_28_-A20FMDV2 and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 at the two time points was 0.49 ± 0.12 and 0.49 ± 0.04% ID/g and 0.52 ± 0.09 and 0.54 ± 0.08% ID/g, respectively. This indicated that PEGylation of the parent compound increased the radioactivity uptake by the tumors; however, introduction of a second PEG molecule in the compound improved the tumor accumulation of the label only marginally.

For the second animal model, the biodistribution of [^18^F]FBA-A20FMDV2, [^18^F]FBA-PEG_28_-A20FMDV2, and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 was investigated in mice bearing BxPC-3 cell tumors (12). In these tumors, the uptake and retention values of [^18^F]FBA-A20FMDV2 at 1 and 4 h were 0.69 ± 0.19 and 0.12 ± 0.03% ID/g, similar to values observed earlier with the DX3puroβ6 tumors. With [^18^F]FBA-PEG_28_-A20FMDV2 and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2, the uptake and retention at these time points was 1.85 ± 0.44 and 1.48 ± 0.04% ID/g, and 1.57 ± 0.25 and 2.08 ± 0.37% ID/g, respectively. Autoradiography of the BxPC-3 xenograft tumors 1 h after treatment with the respective radiolabeled compound confirmed the tumor-specific and favored uptake of the PEGylated radiotracers. For blocking studies, the animals were treated with the corresponding unlabeled PEGylated peptides (30 mg/kg body weight) 10 min before treatment with the labeled peptide version (12). Imaging revealed that the tumor uptake of radioactivity was blocked under these conditions for the labeled mono- (∆SUV_max_ = -77%) and diPEGylated (∆SUV_max_ = -60%) peptides.

The tumor/blood ratios for [^18^F]FBA-A20FMDV2, [^18^F]FBA-PEG_28_-A20FMDV2, and [^18^F]FBA-(PEG_28_)_2_-A20FMDV2 at 4 h after the injection were 7.0, 47.9, and 150, respectively, indicating that PEGylation markedly improved the tumor uptake of the labeled compounds. The tumor/muscle ratios for these labeled tracers at 4 h after treatment were 2.5, 3.6, and 4.4, respectively, suggesting an improved retention of radioactivity with the PEGylated compounds. For all the labeled compounds, the level of radioactivity in the BxPC-3 tumors was at least four-fold higher than the pancreatic tissue itself at all time points, indicating that all these compounds were suitable for detecting α_v_β_6_ integrin–positive tumors in this model. At 4 h after injection, the tumor/normal pancreatic tissue radioactivity retention ratio for [^18^F]FBA-A20FMDV2 was 9.5. These ratios were 23.6 and 4.4 for the mono- and diPEGylated tracers at the same time points, suggesting that [^18^F]FBA-PEG_28_-A20FMDV2 was a better tracer for the detection of α_v_β_6_ integrin–positive tumors than the other two compounds.

MicroPET imaging was performed on mice (n = 3 animals/radiotracer) bearing BxPC-3 cell xenograft tumors at different time points up to 4 h after injecting the animals with the three respective ^18^F-radiolabeled FBA peptides (12). For comparison, another group of animals was imaged as above after treatment with [^18^F]fluorodeoxyglucose ([^18^F]FDG). Tumor uptake of radioactivity was compared as the maximum standard uptake value (SUV_max_) for each tracer. The non-PEGylated peptide had a moderate uptake by the tumors within the first 15 min, but the radioactivity was washed out almost completely by 4 h (SUV_max_ values of 0.50 ± 0.22, 0.22 ± 0.11, and <0.05 at 15 min and at 1 and 4 h, respectively). During the same period, the values were 1.07 ± 0.29, 0.91 ± 0.25, and 0.63 ± 0.12 with a good renal clearance for the mono-PEGylated peptide and 0.99 ± 0.18, 0.79 ± 0.24, and 0.59 ± 0.20 with a high renal retention for the diPEGylated peptide. Under the same conditions, the tumors and the surrounding tissue showed a similar accumulation of radioactivity with [^18^F]FDG, indicating that uptake of the label was nonspecific (12).

With results obtained from the various studies, the investigators concluded that [^18^F]FBA-PEG_28_-A20FMDV2 was a promising agent for the imaging of α_v_β_6_ integrin–positive tumors (12).

### Other Non-Primate Mammals

[PubMed]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FBA+PEG+A20FMDV2+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FBA+PEG+A20FMDV2+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## NIH Support

Some studies mentioned in this chapter were supported by a National Institutes of Health grant R21 CA107792.

## References

1 Bandyopadhyay A., Raghavan S. (2009). Defining the role of integrin alphabeta;alphavbeta6 in cancer. Curr Drug Targets.
2 Heino J., Kapyla J. (2009). Cellular receptors of extracellular matrix molecules. Curr Pharm Des.
3 Breuss J.M., Gallo J., DeLisser H.M., Klimanskaya I.V., Folkesson H.G., Pittet J.F., Nishimura S.L., Aldape K., Landers D.V., Carpenter W., et al. (1995). Expression of the beta 6 integrin subunit in development, neoplasia and tissue repair suggests a role in epithelial remodeling. J Cell Sci.
4 Elayadi A.N., Samli K.N., Prudkin L., Liu Y.H., Bian A., Xie X.J., Wistuba I.I., Roth J.A., McGuire M.J., Brown K.C. (2007). A peptide selected by biopanning identifies the integrin alphavbeta6 as a prognostic biomarker for nonsmall cell lung cancer. Cancer Res.
5 McCarty J.H. (2008). Alphav integrins lead the way for colorectal metastases. Clin Cancer Res.
6 Thomas G.J., Nystrom M.L., Marshall J.F. (2006). Alphavbeta6 integrin in wound healing and cancer of the oral cavity. J Oral Pathol Med.
7 Zhang Z.Y., Xu K.S., Wang J.S., Yang G.Y., Wang W., Wang J.Y., Niu W.B., Liu E.Y., Mi Y.T., Niu J. (2008). Integrin alphanvbeta6 acts as a prognostic indicator in gastric carcinoma. Clin Oncol (R Coll Radiol).
8 Van Aarsen L.A., Leone D.R., Ho S., Dolinski B.M., McCoon P.E., LePage D.J., Kelly R., Heaney G., Rayhorn P., Reid C., Simon K.J., Horan G.S., Tao N., Gardner H.A., Skelly M.M., Gown A.M., Thomas G.J., Weinreb P.H., Fawell S.E., Violette S.M. (2008). Antibody-mediated blockade of integrin alpha v beta 6 inhibits tumor progression in vivo by a transforming growth factor-beta-regulated mechanism. Cancer Res.
9 Hazelbag S., Kenter G.G., Gorter A., Dreef E.J., Koopman L.A., Violette S.M., Weinreb P.H., Fleuren G.J. (2007). Overexpression of the alpha v beta 6 integrin in cervical squamous cell carcinoma is a prognostic factor for decreased survival. J Pathol.
10 Cai W., Niu G., Chen X. (2008). Imaging of integrins as biomarkers for tumor angiogenesis. Curr Pharm Des.
11 Hausner S.H., DiCara D., Marik J., Marshall J.F., Sutcliffe J.L. (2007). Use of a peptide derived from foot-and-mouth disease virus for the noninvasive imaging of human cancer: generation and evaluation of 4-[18F]fluorobenzoyl A20FMDV2 for in vivo imaging of integrin alphavbeta6 expression with positron emission tomography. Cancer Res.
12 Hausner S.H., Abbey C.K., Bold R.J., Gagnon M.K., Marik J., Marshall J.F., Stanecki C.E., Sutcliffe J.L. (2009). Targeted in vivo imaging of integrin alphavbeta6 with an improved radiotracer and its relevance in a pancreatic tumor model. Cancer Res.
13 Sutcliffe-Goulden J.L., O'Doherty M.J., Marsden P.K., Hart I.R., Marshall J.F., Bansal S.S. (2002). Rapid solid phase synthesis and biodistribution of 18F-labelled linear peptides. Eur J Nucl Med Mol Imaging.